# N-Acetyl-N-(2-[^18^F]fluoroethoxybenzyl)-2-phenoxy-5-pyridinamine

Chemical name: | N-Acetyl-N-(2-[^18^F]fluoroethoxybenzyl)-2-phenoxy-5-pyridinamine
Abbreviated name: | [^18^F]FEPPA
Synonym:
Agent Category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR)
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBRs) and peripheral benzodiazepine receptors (PBRs). CBRs are found exclusively in the central nervous system on the membranes of neurons and are coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, PBRs are mitochondrial proteins found in the brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4); the brain has lower levels of PBR than do the peripheral tissues, and both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity. [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart [PuBMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+PK11195)]. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) is a selective agonist used to study PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and ^11^C-labeled DAA1106 ([^11^C]DAA1106) have been developed as potential PET ligands with highly selective and specific binding to PBR. N-Acetyl-N-(2-methoxybenzyl)-2-phenoxy-5-pyridinamine (PBR28), which has an aryloxyanilide structure, has been shown to have high affinity and selectivity for PBR (10). N-Acetyl-N-(2-[^11^C]methoxybenzyl)-2-phenoxy-5-pyridinamine ([^11^C]PBR28) has been developed for imaging PBR in the brain (11). N-Acetyl-N-(2-[^18^F]fluoroethoxybenzyl)-2-phenoxy-5-pyridinamine ([^18^F]FEPPA), an analog of [^11^C]PBR28, is being evaluated as a PET imaging agent for PBR in the brain (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20synthesis)]

Wilson et al. (12) reported the synthesis of [^18^F]FEPPA with ^18^F-fluorination of N-(2-((n-4-phenoxypyridin-3-yl)acetimido)methyl)phenoxy)ethyl 4-methylbenzenesulphonate in acetonitrile solution of K_2_CO_3_/Kryptofix222 for 10 min at 90ºC. [^18^F]FEPPA was purified with high-performance liquid chromatography (HPLC) with radiochemical yields of 50% to 60% in a total synthesis time of 40–50 min. The specific activity was 44.4–99.9 GBq/μmol (1.2–2.7 Ci/μmol) at the end of synthesis with radiochemical purities of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20in%20vitro)]

In vitro [^3^H]PK11195 PBR-binding studies showed that FEPPA and PBR28 had K_i_ values of 0.07 and 0.22 nM, respectively (12). FEPPA has a lipophilicity value (Log D, measured) of 2.99 and little activity against various neurotransmitters and transporters.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20rodentia)]

Wilson et al. performed biodistribution studies in male rats injected with 2–3 MBq (0.054–0.081 mCi) [^18^F]FEPPA (12). The studies showed a modest regional accumulation of radioactivity in the brain with standard uptake values of 0.6 and 0.35 at 5 min and 30 min after injection, respectively. The highest uptake value was exhibited in the olfactory bulb (0.75), followed by the hypothalamus (0.65) and the cerebellum (0.56). The fraction of unchanged [^18^F]FEPPA in the brain as determined with HPLC was >93% at 40 min after injection. The fraction of unchanged [^18^F]FEPPA in plasma samples as determined with HPLC was ~7% at 40 min after injection with one major hydrophilic metabolite. Blocking experiments with co-administration of 0.01–1 mg/kg PBR28 was unsuccessful in terms of the regional and total brain accumulation of radioactivity with a dramatic increase in plasma radioactivity. This may be explained by the observation that binding of [^18^F]FEPPA to peripheral PBR sites was blocked by PBR28, thus increasing the amount of radiotracer in plasma and the amount available to accumulate in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEPPA%20and%20human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Imaizumi M., Kim H.J., Zoghbi S.S., Briard E., Hong J., Musachio J.L., Ruetzler C., Chuang D.M., Pike V.W., Innis R.B., Fujita M. (2007). PET imaging with [11C]PBR28 can localize and quantify upregulated peripheral benzodiazepine receptors associated with cerebral ischemia in rat. Neurosci Lett.
11. Fujita, M., M. Imaizumi, S.S. Zoghbi, Y. Fujimura, A.G. Farris, T. Suhara, J. Hong, V.W. Pike, and R.B. Innis, Kinetic analysis in healthy humans of a novel positron emission tomography radioligand to image the peripheral benzodiazepine receptor, a potential biomarker for inflammation. Neuroimage, 2007.
12 Wilson A.A., Garcia A., Parkes J., McCormick P., Stephenson K.A., Houle S., Vasdev N. (2008). Radiosynthesis and initial evaluation of [(18)F]-FEPPA for PET imaging of peripheral benzodiazepine receptors. Nucl Med Biol.